# ^18^F-Labeled exendin(9-39)

Chemical name: | ^18^F-Labeled exendin(9-39) | [image]
Abbreviated name: | [^18^F]Ex(9-39) | [image]
Synonym: | | [image]
Agent Category: | Peptide | [image]
Target: | Glucagon-like peptide 1 receptor (GLP-1R) | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]Ex(9-39) according to Wang et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glucagon-like%20peptide-1%20receptor&cmd=DetailsSearch)]

Autoimmune processes and other environmental factors that destroy β-cells located in the pancreatic islet cells are known to promote the development of insulin-dependent diabetes mellitus (type 1 diabetes) in individuals genetically predisposed to the disease (2). Due to this destruction, the net mass of the β-cells in the islet cells of the pancreas is reduced, which leads to decreased production of insulin in the individual, and the maintenance of blood glucose at proper physiological levels is impaired. Type 2 diabetes is the most common form of the disease and is primarily caused by insulin resistance as a consequence of low insulin secretion by the β-cells. This form of diabetes can often be corrected with exercise, diet control, and/or medication (3). Upon diagnosis of diabetes, it is important to determine the individual's β-cell mass (BCM) or volume to devise a successful treatment regimen for the condition (4). Changes in the BCM during the onset of diabetes is poorly understood, and an indirect method that measures the amount of stimulated insulin secretion by the pancreas is currently used to quantify the BCM in humans (5). However, the β-cells appear to have a reserved capacity to produce insulin, so the use of insulin secretion as a determinant of BCM is of limited value (5).

As an alternative to determine insulin secretion to quantify BCM, investigators have evaluated the use of noninvasive positron emission tomography (PET) imaging techniques to determine the BCM in rats with the use of ^11^C- or ^18^F-labeled dihydrotetrabenazine, which is an antagonist of the vesicular monoamine transporter type 2 (VMAT2) in the islet cells (6). Careful evaluation of results obtained with the VMAT2 antagonists has revealed that a large proportion of these radiolabeled compounds tend to reside in the exocrine pancreas, indicating that these radiotracers are not suitable for the determination of BCM with PET imaging (7). Recently, some G-protein–coupled receptors (e.g., the glucagon-like peptide 1 (GLP 1) receptor (GLP-1R)), which show a selective location in the β-cells compared to the surrounding exocrine pancreatic cells, were identified by database mining and immunohistochemical staining of pancreatic tissue (1, 7, 8). On the basis of these observations and the known involvement of GLP-1R in β-cell function and biology (for details, see Baggio and Drucker (9)), this receptor was identified as a possible target of radiolabeled probes that can be used to quantify the BCM. Although GLP-1 is the natural ligand for the GLP-1R, a major drawback of using this peptide to measure the BCM is that it is rapidly inactivated by dipeptidyl peptidase, a proteolytic enzyme, while in circulation (half-life, ~2 min). As a consequence, investigators identified and have used radiolabeled Exendin-4 or its analogs (Exendin is a peptide of 39 amino acids that has a 54% homology with GLP-1, acts as an agonist of the GLP-1R with a K_d_ of ~1.4 × 10−^10^ M for this receptor, is not inactivated by proteolytic enzymes, and has a circulation half-life of ~2 h) for the measurement of BCM with noninvasive molecular imaging techniques (1, 7). Connolly et al. evaluated the use of ^64^Cu-labeled Lys^40^(1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid)NH_2_-conjugated Exendin-4 for the in vivo imaging and measurement of the BCM in rats; however, because this tracer accumulated in the kidneys of the rodents, the pancreas was masked in the PET images and the BCM in the animals could not be quantified (7).

Radionuclide-labeled Exendin(9-39) (Ex(9-39)), a truncated version of Exendin, which acts as an antagonist of the GLP-1R and exhibits a high affinity for the receptor (K_d_, ~3 × 10−^9^ M) has also been used by investigators for the visualization of the GLP-1R (1). In an effort to develop a GLP-1R imaging agent, investigators labeled Ex(9-39) with [^18^F]fluoride using N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]FB) (1). However, the ^18^F-succinimidyl ester reacts with all of the primary amine groups available in a peptide, and the final labeled product is a mixture of the labeled peptide molecules that have [^18^F]FB attached randomly on the primary amine groups of amino acids that constitute the peptide. Therefore, the exact structure of ^18^F-labeled FB-conjugated Ex(9-39) is not well defined. In addition, during the labeling reaction the radionuclide may be introduced on an important amine group of the peptide, which can result in the loss of its biological activity. In order to develop a ^18^F-labeled Ex(9-39) with a defined structure, Wang et al. used a site-specific technique to introduce ^18^F into the molecule (1). To achieve this, [^18^F]-4-fluorobenzaldehyde ([^18^F]FBA) was conjugated with a 6-hydrazinonicotinyl group (6-HYNIC) located on the ε-amine of Lys27 in the Ex(9-39) molecule to generate [^18^F]Ex(9-39). To evaluate the GLP-1R imaging ability of the labeled peptide, Sprague-Dawley (SD) rats and BioBreeding diabetes-prone (BB-DP) rats were injected with [^18^F]Ex(9-39), and the time-activity curves for the pancreas, kidney, and the liver of the animals were obtained with PET imaging. Data generated with PET images of the pancreas were then correlated with insulin expressed by β-cells of the organ.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=BCM%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GLP-1R) related to GLP-1R

Gene information (http://www.ncbi.nlm.nih.gov/gene/2740) regarding human GLP-1R (Gene ID: 2740)

Glucagon-like peptide 1 (http://omim.org/entry/138030) in Online Mendelian Inheritance in Man Database (OMIM)

Mouse GLP-1R (http://www.genome.jp/dbget-bin/www_bget?mmu:14652) in Kyoto Encyclopedia of Genes and Genomes Database (KEGG)

GLP-1R agonists for the treatment of type II diabetes: Exenatide (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=751747da-7c1f-41ad-b1a6-a6d920f70599) and Liraglutide (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=5a9ef4ea-c76a-4d34-a604-27c5b505f5a4)

American Diabetes Association (http://www.diabetes.org/)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20synthesis)]

The site-specific ^18^F labeling of Ex(9-39) on the 6-HYNIC moiety on the ε-amine of Lys27 has been described by Wang et al. (1). The identity of [^18^F]Ex(9-39) obtained from the synthesis was confirmed by co-injecting the labeled peptide with non-radiolabeled ^19^F-Ex(9-39) on an analytical size-exclusion high-performance liquid chromatography (HPLC) column. The radiochemical yield (RY) of the labeling reaction was not reported. The radiochemical purity (RP) of [^18^F]Ex(9-39) was usually >95% as determined with HPLC, and the specific activity of the labeled peptide was reported to be ~22.2–25.9 TBq/μmol (~600–700mCi/μmol).

The source, synthesis, RY, RP, and specific activity of ^125^I-labeled Ex(9-39) ([^125^I]Ex(9-39)) used in an in vitro study were not reported (1).

For an ex vivo study, Ex(9-39) was labeled with Cy5.5 (Ex(9-39)-Cy5.5), a near-infrared fluorescent dye, using a commercially available kit (1). The dye:peptide ratio of the conjugate was determined to be ~0.4:1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20in%20vitro&cmd=DetailsSearch)]

To ascertain the β-cell binding selectivity of Ex(9-39), Wang et al. studied the uptake and retention of [^125^I]Ex(9-39) in INS-1 (832/13) cells (a rat insulinoma (http://cancer.gov/dictionary?CdrID=657853) β-cell line) and PANC-1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1469&Template=cellBiology) cells (a human pancreatic exocrine cell line) (1) The normalized uptake and retention of the label was significantly higher (P < 0.01) in the INS-1 cells (34.1 ± 8.0 and 3.0 ± 1.3, respectively) than in the PANC-1 cells (1.4 ± 0.2 and 0.1 ± 0.0, respectively). This indicated that Ex(9-39) had a binding specificity for the β-cells.

In a binding assay of Exendin-Cy5.5 with INS-1 (832/13) cells, it was shown that the fluorescent peptide bound to these cells with specificity and that the binding was saturable (1).

Ex vivo fluorescence imaging of pancreas and liver tissue obtained from mice given an bolus injection of ~40 nmol Ex(9-39)-Cy5.5 showed that the relative fluorescence intensity of the pancreas was ~5-fold higher than that of the liver (1). This indicated that Ex(9-39) bound preferentially to the pancreatic tissue in these animals.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]Ex(9-39) in different organs of SD and BB-DP rats was studied as described elsewhere (1). The SD rats were divided into two groups: a control group (n = 4 animals) and a diabetic group (denoted as STZ for streptozotocin (http://www.emdchemicals.com/life-science-research/streptozotocin/EMD_BIO-572201/p_qpKb.s1LAAoAAAEWhmEfVhTm?PortalCatalogID=merck4biosciences&CountryName=United+States+of+America); n = 6 animals; diabetes in these animals was induced by treatment with STZ, a drug that causes β-cell death). Each rat was injected with ~7 MBq (~0.2 mCi) [^18^F]Ex(9-39) through the tail vein, and dynamic PET images of the animals (under anesthesia) were acquired for the next 180–240 min. The images were reconstructed with appropriate software, and regions of interest on the images were delineated manually for the pancreas, liver, and kidney cortex of the animals. Regional time-activity curves (TAC) were generated from the dynamic PET images to calculate the standardized uptake value (SUV) units after normalization for injected activity and rodent body weight. After the imaging session was over, the animals were euthanized and the pancreas were extracted to determine insulin content.

A high uptake of radioactivity was observed in the myocardium and kidneys of the control SD rats at 10–30 min postinjection (p.i.) (1). The pancreas of these animals showed a low accumulation of label that was similar to the amount in the surrounding tissues, which have a low expression of the GLP-1R. The SUV of the pancreas from animals in all three groups (SD, STZ, and BB-DP) showed a similar and rapid increase in accumulation of label during the initial 10 min p.i.; accumulation peaked at 50 min p.i. and plateaued thereafter. In addition, there was no correlation between the SUV of the pancreas and the postmortem insulin content of these organs. From these observations, the investigators concluded that [^18^F]Ex(9-39) probably did not bind specifically to the GLP-1R in the pancreas (1).

From these studies, it was concluded that ^18^F-labeling of Ex(9-39) on the HYNIC modified Lys27 of the peptide generated a radiolabeled probe that did not bind specifically to the GLP-1R (1). Therefore, this tracer is not suitable for the determination of BCM in rodents.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-Ex9-39%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available

## Supplemental Information

[Disclaimers]

No information is currently available

## NIH Support

Work described in this chapter was published with a CTSA grant (number UL 1 RR024139) from the National Center for Research Resources, a component of the National Institutes of Health (NIH) and NIH roadmap for medical research.

## References

1 Wang Y., Lim K., Normandin M., Zhao X., Cline G.W., Ding Y.S. (2012). Synthesis and evaluation of [(18)F]exendin (9-39) as a potential biomarker to measure pancreatic beta-cell mass. Nucl Med Biol.
2 Concannon P., Rich S.S., Nepom G.T. (2009). Genetics of type 1A diabetes. N Engl J Med.
3 Krentz A.J., Bailey C.J. (2005). Oral antidiabetic agents: current role in type 2 diabetes mellitus. Drugs.
4 Ritzel R.A. (2009). Therapeutic approaches based on beta-cell mass preservation and/or regeneration. Front Biosci.
5 Harris P.E., Ferrara C., Barba P., Polito T., Freeby M., Maffei A. (2008). VMAT2 gene expression and function as it applies to imaging beta-cell mass. J Mol Med (Berl).
6 Kung M.P., Hou C., Lieberman B.P., Oya S., Ponde D.E., Blankemeyer E., Skovronsky D., Kilbourn M.R., Kung H.F. (2008). In vivo imaging of beta-cell mass in rats using 18F-FP-(+)-DTBZ: a potential PET ligand for studying diabetes mellitus. J Nucl Med.
7 Connolly B.M., Vanko A., McQuade P., Guenther I., Meng X., Rubins D., Waterhouse R., Hargreaves R., Sur C., Hostetler E. (2012). Ex Vivo Imaging of Pancreatic Beta Cells using a Radiolabeled GLP-1 Receptor Agonist. Mol Imaging Biol.
8 Cline G.W., Zhao X., Jakowski A.B., Soeller W.C., Treadway J.L. (2011). Islet-selectivity of G-protein coupled receptor ligands evaluated for PET imaging of pancreatic beta-cell mass. Biochem Biophys Res Commun.
9 Baggio L.L., Drucker D.J. (2007). Biology of incretins: GLP-1 and GIP. Gastroenterology.